# ^111^In-CHX-A”-Diethylenetriamine pentaacetic acid-(Z_EGFR:955_)_2_

Chemical name: | ^111^In-CHX-A”-Diethylenetriamine pentaacetic acid-(Z_EGFR:955_)_2_
Abbreviated name: | ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_, ^111^In-(Z_EGFR:955_)_2_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGFR, HER1 receptor
Target category: | Receptor
Method of detection: | SPECT
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody+955)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 operate in three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Cetuximab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER1 (11). Various labeled cetuximab probes have been developed for imaging human breast cancer in small animal tumor models (12-14). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER1, based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A, was constructed (15). The Affibody molecule (Z_EGFR:955_)_2_ exhibits a high binding affinity (K_d_) to HER-expressing cells (K_d_ = 1 nM) (16). (Z_EGFR:955_)_2_ was labeled with ^111^In via CHX-A”-diethylenetriamine pentaacetic acid (DTPA) to form ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_ for single-photon emission computed tomography (SPECT) imaging in nude mice bearing human tumors (17).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody+955)]

CHX-A”-DTPA and (Z_EGFR:955_)_2_ (1:1 molar ratio) were incubated for 20 h at 37°C in sodium borate buffer (pH 9.2). CHX-A”-DTPA-(Z_EGFR:955_)_2_ was isolated from the incubation mixture with a NAP-5 column. CHX-A”-DTPA-(Z_EGFR:955_)_2_ (0.2 M ammonium acetate buffer (pH 5.25)) was mixed with a predetermined amount of ^111^InCl_3_. The mixture was incubated for 1 h at room temperature. A non-binding Affibody was also labeled similarly as a control. No data of labeling efficiency, radiochemical purity, and specific activity for ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_ were reported (17).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody+955%20and%20in%20vitro)]

In vitro binding specificity tests showed that binding of ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_ to human epithelial cancer A431 cells expressing HER1 was mediated by the receptors because saturation of receptors by preincubation with non-labeled (Z_EGFR:955_)_2_ markedly decreased binding of ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_ (17). The cell-bound radioactivity remained at 38% of the initially bound activity for up to 72 h. ^125^I-(Z_EGFR:955_)_2_ was internalized as shown previously with confocal microscopy (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=955%20affibody%20and%20rodentia)]

Nordberg et al. (17) performed biodistribution studies of 0.25 MBq (6.7 μCi) ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_ in nude mice bearing A431 xenografts (n = 4 mice/group). The tracer accumulation values in the A431 tumors were 3.8 ± 1.4% injected dose per gram (ID/g) at 4 h after injection and 2.0 ± 0.5% ID/g at 8 h after injection. The kidneys (86.4% ID/g) and liver (16.5% ID/g) were the only organs that had higher accumulation than the tumor. Blood level was <0.4% ID/g at 4 h, providing a tumor/blood ratio of 9.1. The tumor uptake of the ^111^In-CHX-A”-DTPA-(Z_abeta3:C228S_)_2_ control Affibody was <0.3% ID/g at 4 h. Pre-administration of excess (Z_EGFR:955_)_2_ decreased liver accumulation by 8.2-fold at 4 h after injection, but kidney uptake was approximately doubled. SPECT analysis was performed in nude mice bearing the A431 tumors after intravenous injection of 5 MBq (135 μCi) ^111^In-CHX-A”-DTPA-(Z_EGFR:955_)_2_. The tumor was clearly visualized at 4 h along with the kidneys and liver. Pre-administration of excess (Z_EGFR:955_)_2_ blocked the uptake in the tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody+955%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody+955%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody+955%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Kim E.S., Khuri F.R., Herbst R.S. (2001). Epidermal growth factor receptor biology (IMC-C225). Curr Opin Oncol.
12 Cai W., Chen K., He L., Cao Q., Koong A., Chen X. (2007). Quantitative PET of EGFR expression in xenograft-bearing mice using 64Cu-labeled cetuximab, a chimeric anti-EGFR monoclonal antibody. Eur J Nucl Med Mol Imaging.
13 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
14 Wen X., Wu Q.P., Ke S., Ellis L., Charnsangavej C., Delpassand A.S., Wallace S., Li C. (2001). Conjugation with (111)In-DTPA-poly(ethylene glycol) improves imaging of anti-EGF receptor antibody C225. J Nucl Med.
15 Nord K., Nilsson J., Nilsson B., Uhlen M., Nygren P.A. (1995). A combinatorial library of an alpha-helical bacterial receptor domain. Protein Eng.
16 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
17 Nordberg E., Orlova A., Friedman M., Tolmachev V., Stahl S., Nilsson F.Y., Glimelius B., Carlsson J. (2008). In vivo and in vitro uptake of 111In, delivered with the affibody molecule (ZEGFR:955)2, in EGFR expressing tumour cells. Oncol Rep.
18 Nordberg E., Friedman M., Gostring L., Adams G.P., Brismar H., Nilsson F.Y., Stahl S., Glimelius B., Carlsson J. (2007). Cellular studies of binding, internalization and retention of a radiolabeled EGFR-binding affibody molecule. Nucl Med Biol.